# 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-[^11^C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide

Chemical name: | 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-[^11^C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide
Abbreviated name: | [^11^C]JHU75528
Synonym:
Agent Category: | Compound
Target: | Cannabinoid CB1 receptors
Target Category: | Receptor-ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and some peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominantly in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. The CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid that is found in marijuana and activates CB1 receptors (7). THC has a very high lipophilicity (log D_7.4_ value of 7), which causes imaging studies using radiolabeled THC to be unsuccessful because of slow entry into the brain and high nonspecific binding in the brain. However, a high lipophilicity is essential for binding to CB1 receptors, and an optimal lipophilicity (log D_7.4_ 1–4) is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2, which also exhibit high nonspecific binding and lipophilicity, limiting their application in imaging (8). Therefore, there is a need to lower the lipophilicity of the CB1 radioligands with little effect on binding affinity and ability to cross the BBB. 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide (JHU75528), an analog of SR141716A, is a potent and selective CB1 antagonist with nanomolar affinity and lower lipophilicity than SR141716A (9). 4-Cyano-1-(2,4-dichlorophenyl)-5-(4-[^11^C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([^11^C]JHU75528) is being developed as a positron emission tomography (PET) agent for the non-invasive study of CB1 receptors in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20synthesis)]

Fan et al. (10) reported synthesis of [^11^C]JHU75528 by reaction of the nor-methyl precursor 4-cyano-1-(2,4-dichlorophenyl)-5-(4-hydroxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide with [^11^C]methyl iodide at 80°C in acetone in the presence of 2 M sodium hydroxide. An average radiochemical yield was 16% with a total synthesis time of 28 min after purification by high-performance liquid chromatography. Specific activities were 235 ± 108 GBq/μmol (6.4 ± 2.9 Ci/μmol; n=11) at the end of synthesis with a radiochemical purity of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20in%20vitro)]

Fan et al. (10) reported that JHU75528 had an inhibition constant (K_i_) value of 11 ± 7 nM and a log D_7.4_ (lipophilicity) value of 3.6 ± 0.3. The K_i_ and log D_7.4_ values were 35–46 nM and 4.6 ± 0.8 for SR141716A, respectively. Therefore, JHU75528 displayed higher binding affinity and lower lipophilicity than SR141716A.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20rodentia)]

Horti et al. (9) performed biodistribution studies in male CD-1 mice. Their studies showed that there was a high uptake of radioactivity in the brain after injection of [^11^C]JHU75528. The striatum had the highest accumulation, followed by the hippocampus, cortex, and cerebellum. The brain stem and thalamus had the lowest accumulation. Peak concentration of radioactivity occurred at 15–20 min followed by washout. The striatum/brain stem, hippocampus/brain stem, and cerebellum/brain stem ratios were 3.4, 2.8, and 2.8 at 90 min after [^11^C]JHU75528 injection, respectively. Pretreatment with 2 mg/kg SR141716A and 4 mg/kg JHU75582 15 min before tracer injection reduced the brain uptake to approximately that of background uptake at 60–90 min, whereas various central non-CB1 CNS drugs had marginal effect. After injection of [^11^C]JHU75528 in the mice, 94% and 19% of the total radioactivity in the brain and blood were intact parent compound at 30 min, respectively. There were five hydrophilic metabolites in the blood samples.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20%28primate%20not%20human%29)]

Horti et al. (9) performed a biodistribution PET study in two anesthetized baboons injected with [^11^C]JHU75528 , which showed a rapid accumulation of radioactivity in the brain. Selective maximal uptake was observed in the putamen. The thalamus and pons exhibited lower binding than the other brain regions. The putamen/thalamus and putamen/pons ratios were 2.2 and 2.5 at 90 min, respectively. The peak level of ~4% injected dose (ID)/100 ml was reached in the putamen at 10–20 min. [^11^C]JHU75528 radioactivity was washed out gradually in the putamen to ~3.0% ID/100 ml at 85 min. Using the pons as the reference region, the binding potential (BP) values were estimated for the putamen, caudate, frontal lobe, occipital lobe, and thalamus to be 1.3, 0.85, 0.74, 0.26, and 0.09, respectively. Pretreatment with 1 mg/kg SR141716A 15 min before tracer injection reduced the BP values in the putamen, caudate, frontal lobe, and cerebellum by 55–70%, whereas the binding potential values were reduced by only 20% in the thalamus and 40% in the occipital lobe.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JHU75528%20and%20human)]

No publication is currently available.

## NIH Support

K24 DA00412, R01 AA12839, R01 NS38927

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 3. Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Horti A.G., Fan H., Kuwabara H., Hilton J., Ravert H.T., Holt D.P., Alexander M., Kumar A., Rahmim A., Scheffel U., Wong D.F., Dannals R.F. (2006). 11C-JHU75528: a radiotracer for PET imaging of CB1 cannabinoid receptors. J Nucl Med.
10 Fan H., Ravert H.T., Holt D.P., Dannals R.F., Horti A.G. (2006). Synthesis of 1-(2,4-dichlorophenyl)-4-cyano-5-(4-[11C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([11C]JHU75528) and 1-(2-bromophenyl)-4-cyano-5-(4-[11C]methoxyphenyl)-N-(piperidin-1-yl)-1H-pyrazole-3-carboxamide ([11C]JHU75575) as potential radioligands for PET imaging of cerebral cannabinoid receptor. Journal of Labelled Compounds and Radiopharmaceuticals.